# HiLyte Fluor 647-hyaluronic acid-gold nanoparticles

Chemical name: | HiLyte Fluor 647-hyaluronic acid-gold nanoparticles
Abbreviated name: | HHAuNPs
Synonym:
Agent category: | Glycosaminoglycan
Target: | Hyaluronidase (HAdase)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) imaging
Source of signal: | HiLyte Fluor 647
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle)]

Optical fluorescence imaging is increasingly used to visualize biological functions of specific targets in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (NIRF; 700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIRF imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) consists of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, hyaluronate, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (3). ECM molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (4). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue.

Gold nanoparticles (AuNPs) have been used as X-ray and optical contrast agents in small animals with little toxicity (5). By combining AuNPs and fluorophore, the versatility of Au-fluorophore interactions allows detection of the presence of the AuNPs with fluorescence spectroscopy using NP surface energy transfer (NSET) (6, 7). NSET provides low noise/signal ratios and covers a distance of ~20 nm for metal–fluorophore interactions. Deep tissue imaging can be obtained with the use of NIR dyes. Hyaluronic acid (HA, also known as hyaluronan or hyaluronate) is a high molecular weight linear glycosaminoglycan widely distributed throughout connective, epithelial, and neural tissues and is a hyaluronidase (HAdase) substrate (8-10). The receptor for HA is CD44. HA provides a target for CD44-mediated adhesion of normal and cancer cells (11, 12). Elevated extracellular levels of HA and its partially catabolized oligomers are found in certain malignancies and inflammation (13, 14). Lee et al. (15) conjugated HA with NIR dye HiLyte Fluor 647 to AuNPs (HHAuNPs) for noninvasive detection of reactive oxygen species (ROS) and HAdase activity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle+synthesis)]

Lee et al. (15) produced AuNPs (16 nm) using methods previously reported. Oligo-HA (3–8 kDa) and cystamine hydrochloride were dissolved in borate buffer and incubated with NaBH_3_CN for 5 d at 40°C. The mixture was incubated with dithiothreitol for 12 h to generate free thio groups (87%). End thiol modification of oligo-HA was activated with 1-ethyl-3-(3-dimethylaminopropyl) carbodiimide and reacted with HiLyte Fluor 647 amine to form HiLyte Fluor 647-oligo-HA (HH), which was conjugated to AuNPs to form HHAuNPs. There were 4.5 dye molecules per oligo-HA molecule and 30.9 molecules of oligo-HA per AuNP. The optical properties of HHAuNPs were stable in buffers with pH values 2–12 and serum (Ex/Em, 650/675 nm). The quenching efficiency was estimated to be >96%, mainly caused by the NSET between HH molecules and AuNPs.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle+in+vitro)]

Lee et al. (15) showed that HHAuNPs were activated by ROS (0.1 mM) such as superoxide and hydroxyl radical, as well as HAdase (200 U/ml), with >100-fold increases in NIRF signal after 3 h of incubation. ROS and HAdase caused degradation of the immobilized oligo-HA and thus released the quenching between HA molecules and AuNPS. Lipopolysaccharide and phorbol myristate acetate stimulate THP-1 cells to produce ROS, resulting in 1- to 3-fold increases in fluorescence signals. Cancer cell lines (HTC-116 and OVCAR-3) generated 4- to 6-fold increased fluorescence signals compared with a non-cancer cell line (NIH-3T3). This increase may be the result of cellular secretion of HAdase into the culture medium and the presence of HA receptor (CD44) on the cancer cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle+%20rodentia)]

Lee et al. (15) performed whole-body fluorescence imaging after HHAuNPs (0.5 pmol) were intra-articularly injected into the left forelimbs of both healthy and arthritic mice (n = 4). The NIRF signal was negligible in both healthy and arthritic joints at 30 min after the injection. However, a clearly detectable NIRF signal was observed only in arthritic joints at 2 h after injection. This NIRF signal peaked at 3 h and started to decrease over time. The level of NIRF in the arthritic joint was enhanced ~3.6-fold at 3 h as compared with levels at 30 min after injection. In contrast, no detectable NIRF changes were observed in healthy joints for 12 h. Intravenous injection of HHAuNPs (10 pmol) also showed a 5-fold enhancement in the inflamed regions of the arthritic joints at 6 h after injection. NIRF imaging in mice bearing subcutaneous human ovarian carcinoma (OVCAR-3) tumors detected a NIRF signal near the tumor sites at 6 h after intravenous injection. NIRF signal intensity continued to increase, with a 7.7-fold enhancement near the tumor sites and a 4.8-fold enhancement in the core of tumor at 24 h. Ex vivo examination of Au content and NIRF intensity in the tumor and in five major organs (the liver, spleen, lung, heart, and kidney) revealed that AuNPs and HHAuNPs exhibited a similar distribution pattern except in the tumor, where AuNPs and HHAuNPs resulted in Au levels of 10 and 80 ppm/mg, respectively; the liver had the highest Au content (>120 ppm/mg). On the other hand, the tumor produced the highest NIRF signal, which was 5-fold greater than the liver, which exhibited the second highest NIRF signal. This increase in NIRF signal may be the result of secretion of HAdase into the tumor microenvironment and the presence of the HA receptor (CD44) on the cancer cells. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hyaluronate%20gold%20nanoparticle+human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
4 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
5 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
6 Guarise C., Pasquato L., De Filippis V., Scrimin P. (2006). Gold nanoparticles-based protease assay. Proc Natl Acad Sci U S A.
7 Kim Y.P., Oh Y.H., Oh E., Ko S., Han M.K., Kim H.S. (2008). Energy transfer-based multiplexed assay of proteases by using gold nanoparticle and quantum dot conjugates on a surface. Anal Chem.
8 Caplan, A.I., Embryonic development and the principles of tissue engineering. Novartis Found Symp, 2003249: p. 17-25; discussion 25-33, 170-4, 239-41.
9 Knudson C.B. (2003). Hyaluronan and CD44: strategic players for cell-matrix interactions during chondrogenesis and matrix assembly. Birth Defects Res C Embryo Today.
10 Ward P.D., Thibeault S.L., Gray S.D. (2002). Hyaluronic acid: its role in voice. J Voice.
11 Herrlich P., Morrison H., Sleeman J., Orian-Rousseau V., Konig H., Weg-Remers S., Ponta H. (2000). CD44 acts both as a growth- and invasiveness-promoting molecule and as a tumor-suppressing cofactor. Ann N Y Acad Sci.
12 Naor D., Sionov R.V., Ish-Shalom D. (1997). CD44: structure, function, and association with the malignant process. Adv Cancer Res.
13 Liu D., Pearlman E., Diaconu E., Guo K., Mori H., Haqqi T., Markowitz S., Willson J., Sy M.S. (1996). Expression of hyaluronidase by tumor cells induces angiogenesis in vivo. Proc Natl Acad Sci U S A.
14 Yoshida M., Sai S., Marumo K., Tanaka T., Itano N., Kimata K., Fujii K. (2004). Expression analysis of three isoforms of hyaluronan synthase and hyaluronidase in the synovium of knees in osteoarthritis and rheumatoid arthritis by quantitative real-time reverse transcriptase polymerase chain reaction. Arthritis Res Ther.
15 Lee H., Lee K., Kim I.K., Park T.G. (2008). Synthesis, characterization, and in vivo diagnostic applications of hyaluronic acid immobilized gold nanoprobes. Biomaterials.